# ^99m^Tc-Hexamethylpropyleneamine oxime-blue-biotin-liposomes

Chemical name: | ^99m^Tc-Hexamethylpropyleneamine oxime-blue-biotin-liposomes
Abbreviated name: | ^99m^Tc-HMPAO-BBL
Synonym:
Agent category: | Small molecule (nanoparticle)
Target: | Other
Target category: | Other
Method of detection: | Single-photon emission computed tomography (SPECT)
Source of signal/contrast: | ^99m^Tc
Activation: | No
Studies: | - Rodents; - Non-primate non-rodent mammals | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc-blue-biotine-liposomes)]

The lymphatic system consists of a complex network of lymph vessels, organs, and lymph nodes, and it plays important roles in fluid homeostasis, toxin removal, and immune function (1). Lymph nodes are responsible for filtering lymph fluid and removing foreign materials such as bacteria and cancer cells (2). When lymph nodes become infected or are the sites of tumor metastases, they increase in size. Imaging of a sentinel node, the first lymph node into which the primary tumor drains, can facilitate diagnosis of nodal metastases in cancers (1). Thus, the development of imaging agents to target lymph nodes provokes a great deal of research interest. Colloids that are 2 to 200 nm in length are found to enter into lymphatics through clefts in the lymphatic walls or by endocytosis through the walls (2). After interstitial injection, colloids are transported to the nearest draining lymph node (the sentinel node). The colloids are retained through nonspecific mechanical trapping in the reticular meshwork of the node (2). The trapped colloids are released with time for subsequent migration to other downstream nodes. Lyposomes, a special type of colloid, are used in lymph node–targeted drug delivery and imaging (3). Encapsulation of imaging agents in liposomes increases lymph node targeting and yields enhanced detection sensitivity, for which only a small fraction of liposome-encapsulated labeling is cleared through the lymphatic vessels (3).

The ^99m^Tc-hexamethylpropyleneamine oxime-blue-biotin-liposome (^99m^Tc-HMPAO-BBL) is used for imaging lymphatic nodes with single-photon emission computed tomography (SPECT) (4). ^99m^Tc-HMPAO-BBL consists of biotinylated lipids, liposome-encapsulated ^99m^Tc-HMPAO complexes, and liposome-encapsulated blue dyes. ^99m^Tc is a common radioactive label used in SPECT imaging (5), and it has a 0.90 gamma branch factor, a 6-h half-life at 140 keV, and a low isotope cost ($0.21/mCi) (5). The blue dye, a monosodium salt of 2,5-disulfonated triphenylmethane, has been approved by the United States Food and Drug Administration for clinical lymphangiography (4). HMPAO as a lipophilic chelator carries ^99m^Tc across the lipid bilayer of preformed liposomes that contain reduced glutathione (GSH) (6). In the presence of GSH, ^99m^Tc-HMPAO is chemically reduced to more hydrophilic molecules to be trapped within the liposomal aqueous space (6). This method provides stable ^99m^Tc labeling that is retained within liposomes for prolonged periods without being metabolized. ^99m^Tc-HMPAO-BBL targets lymphatic nodes through a retention mechanism (4) that requires co-injection of avidin, a 68-kDa glycoprotein that has an extraordinarily high affinity for biotin (~10^15^ M^-1^) and can provide four biotin-binding sites. During migration through the lymphatic vessels, biotin-liposomes meet with the avidin, which is also moving into the lymphatic vessels. The association of the biotin-liposomes with avidin results in liposome aggregates. These liposomes aggregate and then become trapped in the first lymph node they encounter, thus prolonging their retention. This method can increase the accumulation of liposomes in lymph nodes from 1–2% to 12% (4). ^99m^Tc-Labeled liposomes in combination with blue dye allow for additive identification of the sentinel lymph node.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(99mTc-blue-biotin-liposomes)+AND+synthesis%0D%0A)]

The synthesis of ^99m^Tc-HMPAO-BBL liposomes was conducted in several steps (4). First, a dry film of liposomes was obtained by mixing lipids in chloroform followed by rotary evaporation and vacuum desiccation. The lipids included distearoyl phosphatidylcholine, cholesterol, N-biotinoyldistearoyl phosphoethanolamine, and α-tocopherol at a molar ratio (total lipid) of 58:39:1:2. Second, the dry film was treated first with a sucrose solution, then with a solution containing a reduced GSH and blue violet dye to produce soluble blue dye–encapsulated liposomes (BBL). This treatment was repeated several times to ensure sufficient encapsulation of sucrose, GSH, and blue dye into the liposomes. BBL had an average diameter of 136 nm and a phospholipid concentration of 29 mM. The intraliposomal concentration of blue dye was found to be 0.15 mg/ml in BBL, corresponding to an encapsulation efficiency of 1.5%. Finally, HMPAO was reacted with a solution containing 370 MBq (10 mCi) ^99m^Tc-sodium pertechnetate. The produced ^99m^Tc-labeled HMPAO was incubated with a concentrated suspension of BBL to yield ^99m^Tc-HMPAO-BBL. The labeling efficiency was found to be 92.1 ± 1.9% by measuring the ^99m^Tc activities with a dose calibrator.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(99mTc-blue-biotin-lipsomes)+AND+%22in+vitro%22%20)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(99mTc-blue-biotin-liposomes)%20+AND++rodentia%20)]

Phillips et al. conducted a biodistribution study of ^99m^Tc-HMPAO-BBL in healthy rats (3). Experimental rats (n = 5; 200–300 g) received intraperitoneal injections of ^99m^Tc-HMPAO-BBL (32.7 mg of phospholipid/kg and 43 MBq of ^99m^Tc), followed by injections of 5 mg avidin (1 ml) in 30 min; the investigators reversed the order in the next two experiments. Control rats (n = 5, 200–300 g) only received ^99m^Tc-HMPAO-BBL. After administration of ^99m^Tc-HMPAO-BBL, whole-body dynamic scintigraphic images were collected per min for 60 min then at 24 h. For the experimental rats, increased accumulation of ^99m^Tc activity was found in the abdominal and mediastinal nodes. Most of the activity was confined to the abdominal region, with virtually no uptake in the spleen. For the control rats, high activity appeared in the spleen, the organ that normally exhibits the highest liposome uptake. After 24 h, 81.9 ± 1.5% of the injected dose was still retained in the experimental animals compared with 72.7 ± 0.20% in the control animals. The distribution of ^99m^Tc-HMPAO-BBL in tissues for the experimental and control rats was 0.17 ± 0.03% and 14.0 ± 1.7% in the blood and 0.78 ± 0.8% and 23.3 ± 3.9% in the spleen, respectively. The experimental group had additional distribution found in the abdominal nodes (4.7%) and mediastinal nodes (2.3%). After the imaging study, rats were euthanized for necropsy and tissue activity counting. The blue staining appeared clearly in the mediastinal and abdominal nodes in experimental rats; no blue-stained nodes were detectable in control rats. The total activity level in the blood and major organs (liver, spleen, kidneys, lungs, and blood) was 51.7% in the control rats versus 9.6% in the experimental rats, which suggested that ^99m^Tc-HMPAO-BBL was easily cleared from the peritoneum and associated lymph nodes in the absence of avidin.

Zavaleta et al. examined regional uptake of ^99m^Tc-HMPAO-BBL in rats with ovarian cancer xenografts (7). Athymic rats were injected with NIH:OVCAR-3 cells in the lower right peritoneal quadrant. The presence of ovarian cancer cells was validated 1 week later with ^18^F-FDG positron emission tomography. Two weeks after inoculation, experimental rats (n = 4) received intraperitoneal injections of 0.3 ml avidin (5 mg) and then 2 ml ^99m^Tc-HMPAO-BBL (38.4 mg of phospholipid/kg and 40.7 MBq of ^99m^Tc) 2 h later. Control rats (n = 3) received only ^99m^Tc-HMPAO-BBL. After injection of ^99m^Tc-HMPAO-BBL, SPECT and computed tomography images were acquired at 4 and 22 h. At 4 h, retention of ^99m^Tc-HMPAO-BBL appeared in the peritoneal cavity, the mediastinal nodes, and the two lymphatic channels that connect the peritoneal cavity and the mediastinal nodes. At 22 h, the experimental rats demonstrated continuous uptake of ^99m^Tc-HMPAO-BBL in the peritoneal activity and the mediastinal nodes. The control rats demonstrated a different distribution pattern in that ^99m^Tc-HMPAO-BBL was rapidly cleared from the peritoneal cavity and accumulated in the spleen at 24 h after injection. The biodistribution of ^99m^Tc-HMPAO-BBL demonstrated that high amounts of uptake occurred in the diaphragm, mediastinal nodes, abdominal nodes, and omentum in the experimental rats. In comparison, liver and spleen uptake was minimal. The result was further confirmed by necropsy with the blue dye staining.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(99mTc-blue-biotin-liposomes)%20+AND+(rabbit+or+dog+or+pig+or+sheep)%20)]

Phillips et al. tracked the migration of ^99m^Tc-HMPAO-BBL toward lymphatic nodes in the presence of avidin in healthy rabbits (n = 6; 2.5–3.0 kg) (4, 8). Rabbits received subcutaneous injections of 0.3 ml ^99m^Tc-HMPAO-BBL (1.5 mg phospholipid/kg and 12 ± 0.9 MBq of ^99m^Tc) on the dorsum of each hind foot. Then 0.3 ml of 5 mg avidin was injected subcutaneously only on the right hind foot (experimental foot) ~2 cm proximal to the injection site of ^99m^Tc-HMPAO-BBL. The left hind foot in each rabbit served as a control. Dynamic scintigraphic images were acquired at 1, 30, and 60 min and again at 24 h. The distribution of ^99m^Tc-HMPAO-BBL was similar in the left and right popliteal lymph nodes at 30 min, but it was different at 60 min and 24 h. The deposition of ^99m^Tc-HMPAO-BBL in the experimental popliteal node and the control popliteal node was 6.5% versus 1.7% at 60 min and 8.5% versus 1.0% at 24 h. The retention efficiency in the experimental leg and the control leg was 20.1% versus 8.5% at 60 min and 17.0% versus 2.5% at 24 h. This was further confirmed with necropsy and radioactivity counting at 24 h after completion of imaging study. In addition, the experimental popliteal node was stained a deep blue color compared to a minimal blue coloration on the control popliteal node. Tissue biodistribution (as percent injected dose per gram (%ID/g)) demonstrated a highly significant increase in liposome deposition in the experimental popliteal node compared with the control popliteal node: 12.2 ± 1.5% ID/g versus 1.2 ± 0.1% ID/g, or 71.4 ± 12.4% ID/g versus 7.4 ± 1.8% ID/g, respectively.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(99mTc-blue-biotin-liposomes)%20+AND+(primate+non+human)%20)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(99mTc-blue-biotin-liposomes)%20+AND+human)]

No publication is currently available.

### NIH Support

EB 000817

## References

1 Barrett T., Choyke P.L., Kobayashi H. (2006). Imaging of the lymphatic system: new horizons. Contrast Media Mol Imaging.
2 Schoder H., Glass E.C., Pecking A.P., Harness J.K., Wallace A.M., Hirnle P., Alberini J.L., Vilain D., Larson S.M., Hoh C.K., Vera D.R. (2006). Molecular targeting of the lymphovascular system for imaging and therapy. Cancer Metastasis Rev.
3 Phillips W.T., Medina L.A., Klipper R., Goins B. (2002). A novel approach for the increased delivery of pharmaceutical agents to peritoneum and associated lymph nodes. J Pharmacol Exp Ther.
4 Phillips W.T., Klipper R., Goins B. (2001). Use of (99m)Tc-labeled liposomes encapsulating blue dye for identification of the sentinel lymph node. J Nucl Med.
5 Yang D.J., Kim E.E., Inoue T. (2006). Targeted molecular imaging in oncology. Ann Nucl Med.
6 Goins B.A., Phillips W.T. (2001). The use of scintigraphic imaging as a tool in the development of liposome formulations. Prog Lipid Res.
7 Zavaleta C.L., Phillips W.T., Soundararajan A., Goins B.A. (2007). Use of avidin/biotin-liposome system for enhanced peritoneal drug delivery in an ovarian cancer model. Int J Pharm.
8 Phillips W.T., Klipper R., Goins B. (2000). Novel method of greatly enhanced delivery of liposomes to lymph nodes. J Pharmacol Exp Ther.